# ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-2-nitroimidazole-N-ethylamine

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-2-nitroimidazole-N-ethylamine
Abbreviated name: | ^68^Ga-NOTA-NI
Synonym:
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Hypoxia
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure (^68^Ga-NOTA-NI) for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI)]

Hypoxia is found in a variety of solid tumors and leads to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized, polarographic, oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7).

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging in 1979 (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic conditions, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). In normoxic conditions, the reduced molecule is rapidly reoxidized and transported from the cell. [^18^F]Fluoromisonidazole ([^18^F]FMISO (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FMISO)) is the most widely used positron emission tomography (10) tracer for imaging tumor hypoxia (7). However, it has slow clearance kinetics and a high lipophilicity, resulting in substantial background in PET scans. [^18^F]Fluoroazomycinarabinofuranoside ([^18^F]FAZA (http://www.ncbi.nlm.nih.gov/books/NBK23282/)) is a 2-nitroimidazole with a sugar addition (11) and has been studied as a hypoxia-imaging agent, showing promising results in various tumor models in rats and mice (12, 13). ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-2-nitroimidazole-N-ethylamine (^68^Ga-NOTA-NI) and ^68^Ga-isothiocyanatobenzyl-1,4,7-triazacyclononane-1,4,7-triacetic acid-2-nitroimidazole-N-ethylamine (^68^Ga-SCN-NOTA-NI) were prepared for hypoxic tissue imaging (14).

### Related Resource Links:

- Chapters in MICAD (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Hypoxia-inducible factor 1, alpha subunit (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3091))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hypoxia (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hypoxia%5BAll+Fields%5D))
- Clinical trials (Hypoxia imaging (http://www.clinicaltrials.gov/ct2/results?term=hypoxia+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI%20and%20synthesis)]

A solution mixture of 2-nitroimidazole-N-ethylamine (0.1 mmol) and NOTA (0.16 mmol) was incubated overnight at room temperature to yield NOTA-2-NI-N-ethylamine (NOTA-NI) (14). NOTA-NI was purified with high-performance liquid chromatography (HPLC). To label with ^68^Ga, a mixture of NOTA-NI and ^68^GaCl_3_ in acetate buffer (pH 5) was heated for 10 min at 100°C. ^68^Ga-NOTA-NI was purified with column filtration. Labeling yields were 96.0 ± 0.7%. ^68^Ga-SCN-NOTA-NI was prepared similarly with labeling yields of 96.3 ± 5.5%. Both agents were stable at room temperature for 4 h with low protein binding. ^68^Ga-NOTA-NI and ^68^Ga-SCN-NOTA-NI are hydrophilic with low partition coefficients (log P) of −0.27 and −0.23, respectively. Radiochemical purity and specific activity of the final product were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI%20and%20in%20vitro)]

In vitro studies indicated that uptake values of both ^68^Ga-NOTA-NI and ^68^Ga-SCN-NOTA-NI in Chinese hamster ovarian (14) cell line (15) and in CT-26 mouse colon cell line xenografts were significantly higher (n = 4, P < 0.05) under hypoxic conditions for 4 h than under normoxic conditions after 60 min of incubation (1.8 ± 0.1 times in CHO, 1.5 ± 0.6 times in CT-26 for ^68^Ga-NOTA-NI; 5.6 ± 1.5 times in CHO, 2.6 ± 0.3 times in CT-26 for ^68^Ga-SCN-NOTA-NI) (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI%20and%20rodentia)]

Ex vivo biodistribution studies of ^68^Ga-NOTA-NI and ^68^Ga-SCN-NOTA-NI in mice (n = 4/group) bearing CT-26 tumors showed a rapid clearance of the tracer from the body over time (10, 30, 60, and 180 min after injection) (14). The highest uptakes were found in the kidneys with 16.43 ± 2.41% injected dose/gram (ID/g) for ^68^Ga-NOTA-NI and 28.53 ± 16.59% ID/g for ^68^Ga-SCN-NOTA-NI at 10 min after injection. The liver and intestine accumulation values of ^68^Ga-SCN-NOTA-NI at 60 min (12.41 ± 1.09 and 9.21 ± 0.72% ID/g, respectively) were higher than those of ^68^Ga-NOTA-NI (3.59 ± 0.21 and 0.66 ± 0.12% ID/g, respectively) at the same time point. The initial tumor uptakes for ^68^Ga-NOTA-NI and ^68^Ga-SCN-NOTA-NI at 10 min after injection were 2.47 ± 0.47 and 2.37 ± 0.29% ID/g , respectively. These radioactivity levels declined over time for both tracers. The tumor/blood ratios for ^68^Ga-NOTA-NI (0.62 ± 0.01) and ^68^Ga-SCN-NOTA-NI (0.73 ± 0.12) at 60 min after injection were lower than those for [^18^F]FAZA (3.27) and [^18^F]FMISO (1.19) at the same time point, whereas the tumor/muscle ratios for ^68^Ga-NOTA-NI (2.13 ± 0.58) and ^68^Ga-SCN-NOTA-NI (1.64 ± 0.39) at 60 min after injection were comparable to those for [^18^F]FAZA (1.69) and [^18^F]FMISO (1.65) at the same time point.

Tumor standardized uptake values (MBq ml^-1^/(ID/weight)) at 30 min and 60 min after injection for ^68^Ga-NOTA-NI (0.52 and 0.30 ± 0.20, respectively) and ^68^Ga-SCN-NOTA-NI (0.35 and 0.19 ± 0.10, respectively) were determined with PET imaging in nude mice bearing CT-26 tumors (14). The tumor/muscle ratios for ^68^Ga-NOTA-NI and ^68^Ga-SCN-NOTA-NI were 5.7 ± 2.5 and 3.95 ± 1.3 at 60 min after injection, respectively. These tumor/muscle ratios were higher than those for [^18^F]FAZA (2.4 ± 0.6) and [^18^F]FMISO (2.7 ± 0.6) at the same time point. ^68^Ga-NOTA-NI and ^68^Ga-SCN-NOTA-NI showed high accumulation in the liver, kidney, and urinary bladder.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NOTA-NI%20and%20humans)]

No publication is currently available.

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Pulkkanen K.J., Laukkanen J.M., Fuxe J., Kettunen M.I., Rehn M., Kannasto J.M., Parkkinen J.J., Kauppinen R.A., Pettersson R.F., Yla-Herttuala S. (2002). The combination of HSV-tk and endostatin gene therapy eradicates orthotopic human renal cell carcinomas in nude mice. Cancer Gene Ther.
11 Reischl G., Ehrlichmann W., Bieg C., Solbach C., Kumar P., Wiebe L.I., Machulla H.J. (2005). Preparation of the hypoxia imaging PET tracer [18F]FAZA: reaction parameters and automation. Appl Radiat Isot.
12 Piert M., Machulla H.J., Picchio M., Reischl G., Ziegler S., Kumar P., Wester H.J., Beck R., McEwan A.J., Wiebe L.I., Schwaiger M. (2005). Hypoxia-specific tumor imaging with 18F-fluoroazomycin arabinoside. J Nucl Med.
13 Sorger D., Patt M., Kumar P., Wiebe L.I., Barthel H., Seese A., Dannenberg C., Tannapfel A., Kluge R., Sabri O. (2003). [18F]Fluoroazomycinarabinofuranoside (18FAZA) and [18F]Fluoromisonidazole (18FMISO): a comparative study of their selective uptake in hypoxic cells and PET imaging in experimental rat tumors. Nucl Med Biol.
14 Hoigebazar L., Jeong J.M., Choi S.Y., Choi J.Y., Shetty D., Lee Y.S., Lee D.S., Chung J.K., Lee M.C., Chung Y.K. (2010). Synthesis and characterization of nitroimidazole derivatives for 68Ga-labeling and testing in tumor xenografted mice. J Med Chem.
15 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.